# ^18^F-6-Fluoro-N-[2-(diethylamino)ethyl]pyridine-3-carboxamide

Chemical name: | ^18^F-6-Fluoro-N-[2-(diethylamino)ethyl]pyridine-3-carboxamide | [image]
Abbreviated name: | ^18^F-MEL050 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Melanin | [image]
Target Category: | Others | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Chemical structure of ^18^F-MEL050 (1, 2).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=benzamide+and+imaging+and+therapy)]

The probe ^18^F-6-fluoro-N-[2-(diethylamino)ethyl]pyridine-3-carboxamide, abbreviated as ^18^F-MEL050, was synthesized by Denoyer et al. for use with melanin-targeted positron emission tomography (PET) of melanoma and its metastasis (1, 2).

Melanoma is a highly malignant tumor that originates in melanocytes. The patient’s outcome is highly dependent on the early detection of metastasis and on the accuracy of staging. Currently, PET with 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) is routinely used for the staging of melanoma, especially for patients with visceral, deep soft tissue, and lymph node metastases (3). However, [^18^F]FDG PET suffers from poor sensitivity for the assessment of early stage and small melanomas because of its dependence on glucose metabolism of tumor cells. Lack of specificity of [^18^F]FDG also makes it difficult to discriminate lymph node metastasis and inflammatory lymphadenopathy (1, 2). In recent years, several other radiolabeled imaging probes have been evaluated for melanoma imaging by targeting melanoma-associated antigens, α-melanocyte–stimulating hormones, and melanin. Of these probes, benzamide (BZ) derivatives are one group of the most promising radiotracers for both diagnosis and therapeutic applications (4, 5).

BZ derivatives represent a versatile class of aromatic compounds that exhibit high and specific binding with melanin in melanoma cells and melanocytes (6, 7). Clinical trials with the agents of [^123^I]BZA and [^123^I]BZA2 have demonstrated the high sensitivity and selectivity of these agents in the detection of melanoma and its metastasis (8-10). Because of the promising results, a large series of BZ derivatives are currently under investigation in animal models of melanoma. In general, these agents exhibit comparable in vitro properties, but they present different kinetic profiles in vivo. Most BZ derivatives exhibit significant liver retention and a predominant clearance via the hepatobiliary system, which potentially limits detection of abdominal lesions (1, 11).

Denoyer et al. synthesized a series of fluoronicotinamide compounds (1, 2, 11). The enhanced hydrophilicity of the pyridine nitrogen allows for rapid clearance of the compounds via renal excretion. The nicotinamide structure is amenable to direct nucleophilic substitution via a rapid, one-step synthesis that provides a means for high-yield incorporation of the ^18^F into these molecules. These ^18^F-labeled compounds, including ^18^F-MEL050, exhibited high radiochemical stability, excellent tumor uptake, and favorable pharmacokinetic properties with excretion predominantly via the renal route (1, 2, 11). These positive characteristics suggest that these agents are potentially valuable as PET agents for early detection of melanoma and its metastasis.

This chapter summarizes the data obtained with ^18^F-MEL050 (1, 2).

### Related Resource Links:

Melanin-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=melanin+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Benzamide derivatives in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pcsubstance&term=benzamide)

Benzamide derivatives in clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=benzamide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Denoyer%20and%20melanoma)]

The agent of ^18^F-MEL050 was prepared from 6-chloro-N-[2-(diethylamino)ethyl]pyridine-3-carboxamide precursor with a one-step radiosynthesis by using no-carrier-added ^18^F-KF-Krytpofix 222 (dimethylformamide, 150ºC, 5 min), followed by purification with high-performance liquid chromatography (1, 2, 11). The synthesis time was 60 min, with an end-of-synthesis yield of 35%–40%, a radiochemical purity of >99%, and a specific activity of 150–220 GBq/µmol (4.05–5.95 Ci)/µmol. The final product was stable (>98%) in saline over 3 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

No data are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Denoyer%20and%20melanoma)]

In one paper published by Denoyer et al., the investigators tested the feasibility of PET imaging with ^18^F-MEL050 in the detection of melanoma and its lung metastasis in animal models (1). The organ uptake was calculated from the PET images and expressed as percent of injected dose per gram of tissue (% ID/g) (assuming a density of 1 g/cm^3^). The background region was chosen to represent the mediastinal blood pool, excluding regions of tracer accumulation such as the spleen.

In a subcutaneous B16-F0 allograft model in C57BL/6 mice (n = 6), PET imaging was performed after tail vein injection of 29.6 MBq (0.8 mCi) ^18^F-MEL050 (1). Images revealed excellent tumor delineation as early as 1 h after injection. The tumor uptake was relatively constant over the 3-h scanning period (9.6 ± 0.5, 9.3 ± 0.7, and 9.0 ± 0.6 at 1, 2, and 3 h, respectively). The tumor/background ratio increased from 19.3 at 1 h to 50.9 at 2 h, reaching 54.3 at 3 h after injection. Accumulation in the bladder, eyes, spleen, and thyroid was visualized, but accumulation in the bone and other organs was not. The radioactivity levels (% ID/g) in the eyes and spleen were also relatively constant, being 2.9 ± 0.2, 2.2 ± 0.1, and 1.7 ± 0.04 in eyes and 3.7 ± 0.4, 2.9 ± 0.4, and 2.6 ± 0.4 in spleen at 1, 2, and 3 h, respectively, after injection. In contrast, the thyroid uptake dropped by >70% between 1 h and 3 h (2.2 ± 0.2 versus 0.6 ± 0.04), rendering the thyroid signal barely detectable at 3 h. Blocking the thyroid by giving mice drinking water supplemented with Lugol's solution for 3 days before ^18^F-MEL050 PET failed to inhibit thyroid uptake (data not shown). The high level of radioactivity in the bladder indicated that ^18^F-MEL050 was rapidly and primarily excreted through the urinary system.

In pigmented and unpigmented melanoma models, PET imaging was performed at 1 h after injection of 22.2 MBq (0.6 mCi) ^18^F-MEL050 to test the specificity of ^18^F-MEL050 (1). Accumulation of the ^18^F-MEL050 was observed in the pigmented B16-F0 tumors in C57BL/6 mice, whereas no significant signal was detected in A375 amelanotic melanoma xenografts in BALB/c nude mice. High-resolution autoradiography of ex vivo tumor sections showed that ^18^F-MEL050 was specifically retained in melanin-containing cells across the entire section of tumor, whereas there was virtually no signal in the unpigmented tumor section. Strong concordance was observed between the ^18^F-MEL050 autoradiographic signals and the brown melanin–pigmented metastasis.

In a B16-BL6 lung metastasis model in BALB/c nude mice (n = 4), mice were imaged on a clinical PET/CT scanner at 1 h after injection of 18–20 MBq (0.49–0.54 mCi) ^18^F-MEL050 (1). Presence of melanoma lesions in the lungs was clearly visualized, and the ^18^F-MEL050 signal in the PET/CT images corresponded to the degree of melanoma invasion of the lung tissue under necroscopy.

For comparison, B16-F0 tumor–bearing mice were scanned with [^18^F]FDG (17.7 MBq (0.48 mCi)) and ^18^F-MEL050 (20.13 MBq (0.54 mCi)), respectively, at 2 h after tracer injection (n = 6 mice) (1). The tumor/background ratio was ~9-fold higher for ^18^F-MEL050 (50.9 ± 6.9) than for [^18^F]FDG (5.8 ± 0.5). ^18^F-MEL050 yielded a much clearer delineation and superior image of melanoma lesions than [^18^F]FDG.

In another paper published by Denoyer et al., the investigators tested the feasibility of using ^18^F-MEL050 in the detection of B16-BL6 metastasis in the left popliteal lymph nodes (PLNs) in C57BL/6 mice (n = 49) (2). PET was performed at 2 h after systemic (20–25 MBq (0.54–0.68 mCi)) (systemic group, n = 24 mice) or subcutaneous perilesional injection (1–1.5 MBq (0.03–0.04 mCi) (local group, n = 25 mice) of ^18^F-MEL050. Mice were euthanized after imaging for ex vivo analysis.

Overall, the radioactive distribution in the mouse body was similar for the two routes of administration, but tracer uptake in the positive PLNs and at the tumor sites was considerably higher in the local group than in the systemic group. ^18^F-MEL050 accumulation was also observed in normal tissues, including the eyes, spleen, thyroid, kidneys, and bladder, with weaker signal in the local group.

The PET scans on day 5 after tumor implantation showed positive PLNs in three of the 24 mice in the systemic group, with node/background ratios of 4.6, 1.9, and 14.0, respectively. Of the 25 mice in local group, five PLNs were judged as positive on the PET scans, and four of the five positive PLNs had uptake ratios between 47 and 68; the remaining PLN (the smallest node) had a ratio of 16. One mouse in the systemic group appeared to have lung metastasis. In the scan on day 9, three more mice in the systemic group and four mice in the local group showed evidence of lung metastases without node involvement. In the scan on day 14, a signal was observed in the subiliac node of a single mouse from the systemic group. The mean uptake level for positive PLNs was 14.2 ± 2.9% ID/g in the systemic group and 197.6 ± 24.4% ID/g in the local group. The mean radioactive level for the negative left PLNs was also higher in the local group (8.5 ± 1.7, n = 16) than in the systemic group (1.7 ± 0.3, n = 15), which may be explained by the fact that more tracers are absorbed into the local lymphatic system and accumulated nonspecifically in the lymph nodes with local injection than with systemic injection. For contralateral PLNs (right side), the level (% ID/g) was almost the same for the two routes of administration (2 ± 0.6 for systemic and 2.7 ± 0.7 for local) on the basis of five pools, each containing three to five right PLNs. The low radioactivity detected in the negative PLNs in both sides may represent the non-specific retention of the agent.

Lymph node metastasis was also examined with ultrasound, confirmed ex vivo under necroscopy, and quantified with ex vivo counting and polymerase chain reaction (PCR)-based tumor burden analysis. Ultrasound correctly identified 90% of positive PLNs, with one false-positive. ^18^F-MEL050 PET correctly identified 60% of positive PLNs after systemic administration and 100% after local administration, with no false-positive results by either route. PET detection efficiency is ~7-fold higher for local than for systemic administrations. The average node/background ratio for positive PLNs was 6.8 in the systemic group and correlated with the PCR-based tumor burden (R^2^ = 0.9764). In the local group, the mean uptake ratio was 48, without clear relation to metastatic burden (R^2^ = 0.1635) (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Denoyer D., Greguric I., Roselt P., Neels O.C., Aide N., Taylor S.R., Katsifis A., Dorow D.S., Hicks R.J. (2010). High-contrast PET of melanoma using (18)F-MEL050, a selective probe for melanin with predominantly renal clearance. J Nucl Med.
2 Denoyer D., Potdevin T., Roselt P., Neels O.C., Kirby L., Greguric I., Katsifis A., Dorow D.S., Hicks R.J. (2011). Improved detection of regional melanoma metastasis using 18F-6-fluoro-N-[2-(diethylamino)ethyl] pyridine-3-carboxamide, a melanin-specific PET probe, by perilesional administration. J Nucl Med.
3 Muller S.P. (2006). Malignant melanoma: PET/CT as a staging procedure. Front Radiat Ther Oncol.
4 Oltmanns D., Eisenhut M., Mier W., Haberkorn U. (2009). Benzamides as melanotropic carriers for radioisotopes, metals, cytotoxic agents and as enzyme inhibitors. Curr Med Chem.
5 Maisonial A., Kuhnast B., Papon J., Boisgard R., Bayle M., Vidal A., Auzeloux P., Rbah L., Bonnet-Duquennoy M., Miot-Noirault E., Galmier M.J., Borel M., Askienazy S., Dolle F., Tavitian B., Madelmont J.C., Moins N., Chezal J.M. (2011). Single photon emission computed tomography/positron emission tomography imaging and targeted radionuclide therapy of melanoma: new multimodal fluorinated and iodinated radiotracers. J Med Chem.
6 Eisenhut M., Hull W.E., Mohammed A., Mier W., Lay D., Just W., Gorgas K., Lehmann W.D., Haberkorn U. (2000). Radioiodinated N-(2-diethylaminoethyl)benzamide derivatives with high melanoma uptake: structure-affinity relationships, metabolic fate, and intracellular localization. J Med Chem.
7 Chezal J.M., Papon J., Labarre P., Lartigue C., Galmier M.J., Decombat C., Chavignon O., Maublant J., Teulade J.C., Madelmont J.C., Moins N. (2008). Evaluation of radiolabeled (hetero)aromatic analogues of N-(2-diethylaminoethyl)-4-iodobenzamide for imaging and targeted radionuclide therapy of melanoma. J Med Chem.
8 Bacin F., Michelot J., Bonafous J., Veyre A., Moreau M.F., Kemeny J.L., Chossat F., Bekhechi D. (1998). Clinical study of [123I] N-(2-diethylaminoethyl)-4-iodobenzamide in the diagnosis of primary and metastatic ocular melanoma. Acta Ophthalmol Scand.
9 Chehade F., De Labriolle-Vaylet C., Michelot J., Moins N., Moreau M.F., Hindie E., Papon J., Escaig F., Galle P., Veyre A. (2001). Distribution of I-BZA (N-2-diethylaminoethyl-4-iodobenzamide) in grafted melanoma and normal skin: a study by secondary ion mass spectroscopy. Cell Mol Biol (Noisy-le-grand).
10 Michelot J.M., Moreau M.F., Veyre A.J., Bonafous J.F., Bacin F.J., Madelmont J.C., Bussiere F., Souteyrand P.A., Mauclaire L.P., Chossat F.M., et al. (1993). Phase II scintigraphic clinical trial of malignant melanoma and metastases with iodine-123-N-(2-diethylaminoethyl 4-iodobenzamide). J Nucl Med.
11 Greguric I., Taylor S.R., Denoyer D., Ballantyne P., Berghofer P., Roselt P., Pham T.Q., Mattner F., Bourdier T., Neels O.C., Dorow D.S., Loc'h C., Hicks R.J., Katsifis A. (2009). Discovery of [18F]N-(2-(diethylamino)ethyl)-6-fluoronicotinamide: a melanoma positron emission tomography imaging radiotracer with high tumor to body contrast ratio and rapid renal clearance. J Med Chem.